# Gadoteridol Gd-HP-DO3A

Chemical name: | Gadoteridol | [image]
Abbreviated name: | Gd-HP-DO3A | [image]
Synonym: | ProHance®, SQ 32692, (10-(2-Hydroxypropyl)-1,4,7,10-tetraazacyclododecane-1,4,7-triacetato)gadolinium, Gadolinium 1,4,7-triscarboxymethyl-1,4,7,10-tetraazacyclododecane | [image]
Backbone: | Compound | [image]
Target: | Non-targeted, central nervous system (CNS), extracranial/extraspinal tissues | [image]
Mechanism: | Blood-brain barrier breakage, perfusion deficiency in extracranial/extraspinal tissues | [image]
Method of detection: | Magnetic resonance imaging (MRI) | [image]
Source of signal /contrast: | Gadolinium (Gd) | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Gadoteridol (C_17_H_29_N_4_O_7_Gd, molecular weight = 558.7). The Gd coordination configuration has not been entirely confirmed by experiments.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22gadoteridol%22%5BSubstance%20Name%5D%20OR%20gadoteridol%5BText%20Word%5D)]

Gadoteridol (Gd-HP-DO3A) is a paramagnetic contrast agent of magnetic resonance imaging (MRI) (1-4). It is approved by the United States Food and Drug Adminsitration (US FDA) for visualization of lesions in the central nervous system (CNS) and extracranial/extraspinal tissues (1).

Conventional, water-soluble paramagnetic contrast agents are generally metal chelates with unpaired electrons, and they work by shortening both T_1_ and T_2_ relaxation times of surrounding water protons to produce the contrast-enhancing effect. At low doses, the T_1_ effect tends to dominate (2, 3). Current clinical agents are water-soluble compounds that do not cross the intact blood-brain barrier (BBB).They can be used to enhance signals of CNS tissues that lack a BBB (e.g., pituitary gland), extraaxial tumors (e.g., meningiomas), and areas of BBB breakdown (e.g., tumor margins) (5-8). In these cases, small or multiple CNS lesions are more clearly delineated with contrast enhancement. In addition, contrast enhancement can highlight vasculature, delineate the extent of disease, and confirm the impression of normal or nonmalignant tissues. These contrast agents can also be used in a similar nonspecific manner to enhance contrast between perfused and nonperfused areas in other organs, such as the liver and myocardium (2-4).

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective at enhancing proton relaxation because of its high magnetic moment and very labile water coordination (3, 5, 6). Gd-DTPA (gadopentetate dimeglumine) was the first intravenous MRI contrast agent used clinically, and a number of similar gadolinium based contrast agents (GBCAs) have been developed in an effort to further improve clinical efficacy, patient safety and patient tolerance. The major chemical differences among these Gd chelates are the presence or absence of overall charge, ionic or nonionic, and their ligand frameworks (linear or macrocyclic) (5, 7). Whereas Gd-DTPA is an ionic linear chelate, Gd-HP-DO3A has a macrocyclic tetraamine framework and is nonionic. Because of these differences, Gd-DTPA(0.5 M) possesses an osmolality of 1940 mOsmol/kg with a 1:3 ratio of Gd atoms to solute particles, but Gd-HP-DO3A in the same concentration has an osmolality of 630 mOsm/kg and a Gd:solute ratio of 1:1.

The commercial formulation (http://www.bracco.com/usa/en-US/Imaging/MRI/ProHance/) of gadoteridol is available as a 0.5 M injection with a recommended dose of 0.1 mmol/kg(0.2 ml/kg) either as a rapid intravenous infusion or bolus injection for CNS or head/neck MRI imaging (1). A second dose of 0.2 mmol/kg (0.4 ml/kg) of the commercial product may be given up to 30 min after the first dose.

Both renal and extra-renal toxicities have been reported following the clinical use of gadolinium in patients with underlying kidney disease (8-10). In 2007, the US FDA (http://www.fda.gov/cder/drug/infopage/gcca/default.htm) requested manufacturers of all GBCAs to add new warnings about exposure to GBCAs increases the risk for nephrogenic systemic fibrosis (NSF) in patients with advanced kidney disease.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22gadoteridol%22%5BSubstance%20Name%5D%20OR%20gadoteridol%5BText%20Word%5D%29%20AND%20synthesis%5BAll%20Fields%5D)]

The macrocyclic DO3A and R-DO3A ligands were synthesized by Dischino and colleagues (11) in 1991. There were several pathways for the synthesis of the DO3A core ligand. The most direct synthesis involved the alkylation of the commercially available unprotected cyclen, 1,4,7,10-tetraazacyclododecane, with chloroacetic acid to give a final yield of 26.2%. Several other multistep synthesis approaches were possible. The most productive approach (69% yield) appeared to be preparing the formyl cyclen, 10-formyl-1,4,7,10-tetraazacyclododecane-1,4,7-triacetic acid, tris-(1,1-dimethylethyl)ester, in which the protecting groups could be easily removed. In this approach, HP-DO3A was first prepared by reacting DO3A with N-(2-hydroxy-ethyl)-2-chloroacetamide in sodium hydroxide. HP-DO3A was then reacted with gadolinium oxide at pH 4.0 and 100^o^C for 5 h. After preparative high performance liquid chromatography (HPLC) purification, the final yield of Gd-HP-DO3A was 43%.

The commercial preparation of Gd-HP-DO3A contains 279.3 mg of gadoteridol/ml with a pH of 6.5-8.0, viscosity of 1.3 cP at 37^o^C, specific gravity of 1.140 at 25^o^C, and an octanol:H_2_O coefficient of −3.68 ± 0.02 (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22gadoteridol%22%5BSubstance%20Name%5D%20OR%20gadoteridol%5BText%20Word%5D%29%20AND%20%28%22in%20vitro%22%5BMeSH%20Terms%5D%20OR%20in%20vitro%5BText%20Word%5D%29)]

The in vitro relaxivity value of Gd-HP-DO3A, ^20^r_1_ (T_1_ relaxivity at 20 MHz), was determined to be 3.7 ± 0.1 (mM−^1^s−^1^) with a Q (the number of simultaneously coordinated water molecules) = 1.3 ± 0.1 and a rotational correlation time(τ_R_) of 57 ps (5). In comparison, the value of ^20^r_1_ for Gd-DTPA was 3.8 ± 0.1 mM−^1^s−^1^.

An in vitro erythrocyte compatability test indicated that 0.5 M Gd-HP-DO3A did not appear to have any potential to hemolyze human erythrocytes (12). An acute cardiotoxicity study in the isolated rat heart model showed only small inotropic and electrophysiologic effects induced by Gd-HP-DO3A at 0.3-1.5 mmol/kg of body weight doses (13). The conditional stability constant (Log K’ at pH 7.4) of Gd-HP-DO3A was 17.1 (5). In another qualitative comparison study of various Gd chelates, Gd-HP-DO3A was found to be kinetically very inert (transmetallation kinetics with Zn^2+^) (14). Inhibition of the angiotensin-converting enzyme (ACE; a zinc- dependent metallopeptidase) by Gd-HP-DO3A was 7.7 ± 1.9 mM/l (LC_50_) (15).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22gadoteridol%22%5BSubstance%20Name%5D%20OR%20gadoteridol%5BText%20Word%5D%29%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%29)]

The acute intravenous LD_50_s (mmol/kg) for 0.5 M Gd-HP-DO3A were 11-14 in mice and >10 in rats (12). In a local tissue toxicity study using mice, Gd-HP-DO3A appeared to cause less tissue damage in response to extravascular extravasation than ionic contrast agents (16). Geschwind and colleagues (22) studied acute hemodynamic effects of contrast agents in rats and found that Gd-HP-DO3A at doses of 0.25-0.5 mmol/kg induced cardiovascular changes that were only slightly less profound than those produced by Gd-DTPA.

In rat biodistribution studies, Gd-153-labeled GD-HP-DO3A was largely distributed in extracellular space, renally excreted, and did not cross the BBB (17, 18). More than 90% of the dose appeared in the urine within 4 h of injection (25). Tissue concentrations indicated a linear function of injected doses in blood, skeletal muscle, and myocardium. MR signals (T_1_-weighted, spin-echo pulse sequence) from imaging increased with increasing tissue concentrations up to 0.61 µmol/g in heart and 0.63 µmol/g in skeletal muscle. Above these concentrations, MR signals did not increase further. The residual whole-body Gd retention in mice and rats of Gd-HP-DO3A also appeared to be lower than that of Gd-DTPA (25, 26).

Using a rat brain gliosarcoma model, Runge and colleagues (19) demonstrated that Gd-HP-DO3A provided MRI enhancement in brain tissue with an altered BBB to allow identification of the implanted tumor lesion.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gadoteridol%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

A 2-week intravenous study (0.5 M) in dogs indicated no treatment-related changes and no treatment-related lesions at dose levels of 0.25-1.5 mmol/kg (12). Only bleeding times and serum iron levels appeared to have slight transient changes after repeated doses. Gd-HP-DO3A at 1.0 M was maternotoxic in rabbits at doses of 6 mmol/kg. No neutrotoxicity was observed in rabbits with induced breakdown of the BBB for 6 weeks after receiving i.v. 0.3 mmol/kg of Gd-HP-DO3A (20).

Gd-HP-DO3A was rapidly cleared from the dog blood, and about 88% of the injected dose was excreted in the urine within 24-48 hours (21). With the use of MRI and direct brain ventricular injection in guinea pigs with induced hydrocephalus, Yamada and colleagues (22) found that Gd-HP-DO3A moved in the CSF in proportion to the CSF pressure. It was observed to clear from the lateral and third ventricles, but it was not observed to reach either over the convexity of the brain or adjacent to the superior sagittal sinus. The detectability of brain metastases with Gd-HP-DO3A was studied in a rabbit brain tumor model. The use of a higher dose (0.3 mmol/kg) appeared to improve metastatic lesion detectability from 30 ± 15% of 0.1 mmol/kg to 104 ± 10%. Other studies in rabbits and dogs showed that the use of this agent could also be valuable in other organ systems [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gadoteridol%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)].

### Non-Human Primates

[[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gadoteridol%20AND%20%28primate%20NOT%20human%29)]

The distribution of Gd-HP-DO3A in healthy rhesus monkeys was used in a number of studies as a control for comparison with newer MRI contrast agents [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gadoteridol%20AND%20%28primate%20NOT%20human%29)].

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gadoteridol%20AND%20human)]

In the United States, a Phase I clinical trial with 18 healthy male volunteers (18-40 years of age) showed that gadoteridol (0.05-0.3 mmol/kg) rapidly distributed from the vascular compartment to the extracellular fluid space, and it was excreted by glomerular filtration in the kidneys (23). About 94 ± 4.8% of the injected dose was excreted in the urine within 24 h. The elimination and distribution half-lives were independent of the doses used in the study. The mean distribution and elimination half-lives were 0.20 ± 0.04 and 1.57 ± 0.08 h, respectively. Adult patients (n=87) with intracranial tumors were studied in the phase II clinical trial to determine the safety of Gd-HP-DO3A at doses of 0.025, 0.05, 0.10, 0.15, 0.20 and 0.30 mmol/kg (6). Gadoteridol was well tolerated with no significant adverse reactions within the studied dose range.

The Phase III clinical trial of Gd-HP-DO3A, at a dose of 0.10 mmol/kg in the United States, was a multicenter (27 sites) study involving patients (n=411) suspected of having intracranial or spinal pathology (24). MRI imaging (1.5 Tesla MRI) was used to produce precontrast (both T_1_- and T_2_-weighted) scans and postcontrast (T_1_-weighted) scans, and blinded evaluation was conducted by two readers. Improved contrast enhancements were observed in 62-83% of the cases, and in 43-76% of the cases, additional diagnostic information was provided. In comparison, the European Phase III multicenter trial with 151 patients using unblinded investigators showed improved contrast enhancement in 75% of cases with brain pathology and 64% of cases involving spine lesions (25). In a U.S. pediatric patient study, the agent was found to be equally safe and improved contrast enhancement was present in 77% (n=22) of the cases (26). Comparison studies generally indicated that the clinical performance of Gd-HP-DO3A for CNS imaging was comparable with other commercially available agents (27, 28).

Runge and Parker (29) reported a worldwide clinical safety assessment of gadoteridol in 1997 that indicated a 6.6% incidence rate of total adverse events (nausea, taste perversion, headache, etc.) from 2656 administered injections in Europe and the United States. Gibby and colleagues (30) in 2004 found that Gd-HP-DO3A had a relatively low Gd retention in human bone tissue (0.466 ± 0.387 µg/g) after the administration of a clinical dose to eight patients.

## Supplemental Information

[Disclaimers]

Gadoteridol package insert

## References

1 ProHance (Gadoteridol Injection) Package Insert2002: Bracco Diagnostics Inc. F1/3.5281.96.
2 Brasch, R.C., M.D. Ogan and B.L. Engelstad, Paramagnetic Contrast Agents and Their Application in NMR Imaging, in Contrast media; Biologic effects and clinical application, Z. Parvez, R., R. Monada and M. Sovak, Editor. 1987, CRC Press, Inc.: Boca Raton, Florida. p. 131-143.
3 Saini, S., J.T. Ferrucci, Enhanced Agents for Magnetic Resonance Imaging: Clinical Applications, in Pharmaceuticals in Medical Imaging, D.P. Swanson, H.M. Chilton and J.H. Thrall, Editor. 1990, MacMillan Publishing Co., Inc.: New York. p. 662-681.
4 Runge V.M., Kirsch J.E., Wells J.W., Awh M.H., Bittner D.F., Woolfolk C.E. (1993). Enhanced liver MR: Contrast agents and imaging strategy. Critical Reviews in Diagnostic Imaging.
5 Tweedle M.F. (1997). The ProHance story: the making of a novel MRI contrast agent. Eur Radiol.
6 DeSimone, D., M. Morris, C. Rhoda, T. Lucas, J. Zielonka, A. Olukotun, and M. Carvlin, Evaluation of the safety and efficacy of gadoteridol injection (a low osmolal magnetic resonance contrast agent). Clinical trials report. Invest Radiol, 199126 Suppl 1: p. S212-6; discussion S232-5.
7 Runge V.M. (2000). Safety of approved MR contrast media for intravenous injection. J Magn Reson Imaging.
8 Perazella M.A., Rodby R.A. (2007). Gadolinium use in patients with kidney disease: a cause for concern. Semin Dial.
9 Grobner, T. and F.C. Prischl, Gadolinium and nephrogenic systemic fibrosis. Kidney Int, 2007
10 Pedersen M. (2007). Safety update on the possible causal relationship between gadolinium-containing MRI agents and nephrogenic systemic fibrosis. J Magn Reson Imaging.
11 Dischino D.D., Delaney E.J., Emswiler J.E., Gaughan G.T., Prasad J.S., Srivastava S.K., Tweedle M.F. (1991). Synthesis of nonionic gadolinium chelates useful as contrast agents for magnetic resonance imaging. Inorg. Chem.
12 Soltys R.A. (1992). Summary of preclinical safety evaluation of gadoteridol injection. Invest Radiol.
13 Akre B.T., Dunkel J.A., Hustvedt S.O., Refsum H. (1997). Acute cardiotoxicity of gadolinium-based contrast media: findings in the isolated rat heart. Acad Radiol.
14 Puttagunta N.R., Gibby W.A., Puttagunta V.L. (1996). Comparative transmetallation kinetics and thermodynamic stability of gadolinium-DTPA bis-glucosamide and other magnetic resonance imaging contrast media. Invest Radiol.
15 Corot C., Idee J.M., Hentsch A.M., Santus R., Mallet C., Goulas V., Bonnemain B., Meyer D. (1998). Structure-activity relationship of macrocyclic and linear gadolinium chelates: investigation of transmetallation effect on the zinc-dependent metallopeptidase angiotensin-converting enzyme. J Magn Reson Imaging.
16 Runge V.M., Dickey K.M., Williams N.M., Peng X. (2002). Local tissue toxicity in response to extravascular extravasation of magnetic resonance contrast media. Invest Radiol.
17 Tweedle M.F., Wedeking P., Telser J., Sotak C.H., Chang C.A., Kumar K., Wan X., Eaton S.M. (1991). Dependence of MR signal intensity on Gd tissue concentration over a broad dose range. Magn Reson Med.
18 Wedeking P., Sotak C.H., Telser J., Kumar K., Chang C.A., Tweedle M.F. (1992). Quantitative dependence of MR signal intensity on tissue concentration of Gd(HP-DO3A) in the nephrectomized rat. Magn Reson Imaging.
19 Runge V.M., Kaufman D.M., Wood M.L., Adelman L.S., Jacobson S. (1989). Experimental trials with Gd(DO3A)--a nonionic magnetic resonance contrast agent. Int J Rad Appl Instrum B.
20 Evill C.A., Wilson A.J., Fletcher M.C., Sage M.R. (1996). Neurotoxicity of contrast media for magnetic resonance imaging after generalized breakdown of the blood-brain barrier. Acad Radiol.
21 Eakins M.N., Eaton S.M., Fisco R.A., Hunt R.J., Ita C.E., Katona T., Owies L.M., Schramm E., Sulner J.W., Thompson C.W., et al. (1995). Physicochemical properties, pharmacokinetics, and biodistribution of gadoteridol injection in rats and dogs. Acad Radiol.
22 Yamada S., Shibata M., Scadeng M., Bluml S., Nguy C., Ross B., McComb J.G. (2005). MRI tracer study of the cerebrospinal fluid drainage pathway in normal and hydrocephalic guinea pig brain. Tokai J Exp Clin Med.
23 McLachlan S.J., Eaton S., De Simone D.N. (1992). Pharmacokinetic behavior of gadoteridol injection. Invest Radiol.
24 Runge, V.M., R.A. Bronen and K.R. Davis, Efficacy of gadoteridol for magnetic resonance imaging of the brain and spine. Invest Radiol, 199227(August Supplement): p. S22-S32.
25 Seiderer M. (1992). Phase III clinical studies with gadoteridol for the evaluation of neurologic pathology. A European perspective. Invest Radiol.
26 Debatin J.F., Nadel S.N., Gray L., Friedman H.S., Trotter P., Hockenberger B., Oakes W.J. (1992). Phase III clinical evaluation of gadoteridol injection: experience in pediatric neuro-oncologic MR imaging. Pediatr Radiol.
27 Greco A., Parker J.R., Ratcliffe C.G., Kirchin M.A., McNamara M.T. (2001). Phase III, randomized, double-blind, cross-over comparison of gadoteridol and gadopentetate dimeglumine in magnetic resonance imaging of patients with intracranial lesions. Australas Radiol.
28 Yuh W.T., Fisher D.J., Engelken J.D., Greene G.M., Sato Y., Ryals T.J., Crain M.R., Ehrhardt J.C. (1991). MR evaluation of CNS tumors: dose comparison study with gadopentetate dimeglumine and gadoteridol. Radiology.
29 Runge V.M., Parker J.R. (1997). Worldwide clinical safety assessment of gadoteridol injection: an update. Eur Radiol.
30 Gibby W.A., Gibby K.A., Gibby W.A. (2004). Comparison of Gd DTPA-BMA (Omniscan) versus Gd HP-DO3A (ProHance) retention in human bone tissue by inductively coupled plasma atomic emission spectroscopy. Invest Radiol.